# Gadolinium-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys

Chemical name: | Gadolinium-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys
Abbreviated name: | Gd-DOTA-R832
Synonym:
Agent category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DOTA-R832)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Endothelial cells are important cells in inflammatory responses (2, 3). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (4).

VCAM-1 is found in very low amounts on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (5-9). VCAM-1 binds to the very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (10). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression to vulnerable plaques, which may erode and rupture. CLIO nanoparticles targeted with anti-VCAM-1 antibody are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (11). A cyclic peptide, Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys (R832), was identified with phage screening against VCAM-1 (12). Gd-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (Gd-DOTA) was conjugated to the N-terminus of R832 to form Gd-DOTA-R832 with a squarate group as a linker. Gd-DOTA-R832 is being developed as a non-invasive MRI agent for VCAM-1 expression in vascular endothelial cells in atherosclerosis.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=VCAM-1)
- Clinical trials (VCAM-1 (http://www.clinicaltrials.gov/ct2/results?term=VCAM-1))
- Drug information in FDA (http://google2.fda.gov/search?q=VCAM-1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=11)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+synthesis)]

The synthesis of Gd-DOTA-R832 was described by Burtea et al. (12). R832 with the Lys residue protected with trifluoroacetic acid (250 mg) was added to Gd-DOTA-diethylsquarate (210 mg) at pH 8.5 and incubated for 4 days. The peptide was deprotected by hydrolysis (pH 9.5) at room temperature for 2 h. Gd-DOTA-R832 was isolated with high-performance liquid chromatography and confirmed with mass spectroscopy. A scrambled peptide (R832.Sc) was also conjugated with Gd-DOTA as a control. Gd-DOTA-R832, Gd-DOTA-R832.Sc, and Gd-DOTA exhibited longitudinal (r_1_) relaxivity values of 8, 8, and 3 mM^-1^s^-1^ at 60 MHz, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+in+vitro)]

Burtea et al. (12) measured the binding affinity of R832 to human VCAM-1 with a dissociation constant (K_d_) of 103 nM. In vitro cell adhesion assays to human VCAM-1 with R832 using Jurkat cells exhibited a 50% inhibition concentration (IC_50_) value of 630 nM. Anti-VCAM-1 antibody showed an IC_50_ value of 1,350 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+rodentia)]

Burtea et al. (12) performed in vivo MRI in apolipoprotein E–deficient (apoE^-/-^) mice after injection with Gd-DOTA-R832 (n = 8), Gd-DOTA-R832.Sc (n = 4), or Gd-DOTA (n = 5). There was 110% enhancement in MRI signal intensity (ΔSNR) in the aortic wall at 10 min after injection. The ΔSNR remained constant (87%) for up to 60 min of imaging. Gd-DOTA-R832.Sc exhibited ΔSNR of 73% and 53% at 10 and 60 min, respectively. Gd-DOTA produced ΔSNR of 71% and 28% at 10 and 60 min, respectively. Pretreatment with R832 15 min before Gd-DOTA-R832 injection reduced the enhancement by ~50% at 42 min after injection. In control normal mice, Gd-DOTA-R832 produced little enhancement in the aortic wall. Immunohistological staining of the aorta sections of apoE^-/-^ mice confirmed the presence of atherosclerotic lesions with extensive expression of VCAM-1. R832 colocalized with VCAM-1 expression. In mice with ConA hepatitis, Gd-DOTA-R832 (n = 9) showed ΔSNR of 60% and 55% at 15 and 60 min after injection, respectively. In contrast, Gd-DOTA (n = 6) showed ΔSNR of 39% to 47% during the first 7 min and ΔSNR of ~15% at 60 min after injection. Gd-DOTA-R832 (n = 6) and Gd-DOTA (n = 7) showed ΔSNR of <10% at 50–60 min after injection in normal mice. R832 colocalized with VCAM-1 expression in the hepatitis liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DOTA-R832+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
5 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
6 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
7 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
8 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
9 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
10 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
11 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.
12 Burtea C., Laurent S., Port M., Lancelot E., Ballet S., Rousseaux O., Toubeau G., Vander Elst L., Corot C., Muller R.N. (2009). Magnetic resonance molecular imaging of vascular cell adhesion molecule-1 expression in inflammatory lesions using a peptide-vectorized paramagnetic imaging probe. J Med Chem.